# ^125^I-Labeled mesenchymal-epithelial transition factor binding peptide-Gly-Gly-Gly

Chemical name: | ^125^I-Labeled mesenchymal-epithelial transition factor binding peptide-Gly-Gly-Gly | Lys-Ser-Leu-Ser-Arg-His-Asp-His-Ile-His-His-His-Gly-Gly-Gly-Ser-Cys
Abbreviated name: | [^125^I]cMBP-GGG | Lys-Ser-Leu-Ser-Arg-His-Asp-His-Ile-His-His-His-Gly-Gly-Gly-Ser-Cys
Synonym: | | Lys-Ser-Leu-Ser-Arg-His-Asp-His-Ile-His-His-His-Gly-Gly-Gly-Ser-Cys
Agent Category: | Ligand | Lys-Ser-Leu-Ser-Arg-His-Asp-His-Ile-His-His-His-Gly-Gly-Gly-Ser-Cys
Target: | Mesenchymal-epithelial transition factor receptor (c-Met); hepatocyte growth factor receptor (HGFR) | Lys-Ser-Leu-Ser-Arg-His-Asp-His-Ile-His-His-His-Gly-Gly-Gly-Ser-Cys
Target Category: | Receptor | Lys-Ser-Leu-Ser-Arg-His-Asp-His-Ile-His-His-His-Gly-Gly-Gly-Ser-Cys
Method of detection: | Single photon-emission computed tomography (SPECT); gamma planar imaging | Lys-Ser-Leu-Ser-Arg-His-Asp-His-Ile-His-His-His-Gly-Gly-Gly-Ser-Cys
Source of signal / contrast: | ^125^I | Lys-Ser-Leu-Ser-Arg-His-Asp-His-Ile-His-His-His-Gly-Gly-Gly-Ser-Cys
Activation: | No | Lys-Ser-Leu-Ser-Arg-His-Asp-His-Ile-His-His-His-Gly-Gly-Gly-Ser-Cys
Studies: | - In vitro; - Rodents | Structure of cBMP-GGG.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cMBP-GGG-Cy5.5)]

The hepatocyte growth factor (HGF) is the only known ligand of the mesenchymal-epithelial transition factor (c-Met) (also known as the HGF receptor) that has an important function, including cell development, proliferation, scattering, migration, and angiogenesis, all of which are necessary for the survival and repair of tissues (1). c-Met is known to mediate its activity through an intracellular tyrosine kinase (TK) that activates different signal transduction pathways leading to initiation of the various cell processes (2). Also, deregulation of c-Met activity due to paracrine/autocrine activation, overexpression, or a mutation promotes the development of a neoplastic cell phenotype (2). Overexpression of c-Met and HGF has been associated with a poor prognosis and survival of the patient (3), suggesting that the c-Met receptor may be a suitable target for the detection of cancers at an early stage, which could help in the development of an appropriate treatment regimen to improve patient prognosis (4). c-Met is the target of several drugs under evaluation in clinical trials (http://clinicaltrials.gov/ct2/results?term=HGFR) approved by the United States Food and Drug Administration. Investigators recently generated a monoclonal antibody (mAb) that inhibits the HGF–c-Met interaction and identified the active mAb cell-surface epitope peptide as KSLSRHDHIHHH, which was designated as the c-Met binding peptide (cMBP) (5). The cMBP and its derivatives (containing a tri-amino acid linker, Gly-Gly-Gly (GGG), or an aliphatic carbon linker, 8-aminooctanoic acid (AOC)) were labeled with ^125^I to generate ^125^I-cMBP, 1^25^I-cMBP-GGG, and ^125^I-cMBP-AOC, and these agents were used to detect c-Met TK-positive tumor xenografts in mice (6). From this study the investigators concluded that although ^125^I-cMBP-GGG was suitable for the imaging of c-Met TK-expressing tumors, the signal to background ratio obtained from this nuclide was not very strong, and the results could probably be improved by using another radionuclide or by modifying the linkers.

In an attempt to generate a c-Met–positive tumor imaging agent superior to ^125^I-cMBP, ^125^I-cMBP-GGG, and ^125^I-cMBP-AOC, investigators conjugated a near-infrared (NIR) fluorescent dye, cyanine 5.5 (Cy5.5), to cMBP-GGG and cMBP-AOC to obtain cMBP-GGG-Cy5.5 and cMBP-AOC-Cy5.5 (4). The Cy5.5-conjugated cMBP derivatives were then evaluated for the NIR imaging of c-Met–positive xenograft tumors in a mouse model.

This chapter describes the in vitro and in vivo characterization of only ^125^I-cMBP-GGG. The other c-Met imaging agents (1^25^I-cMBP, ^125^I-cMBP-AOC, cMBP-GGG-Cy5.5, and cMBP-AOC-Cy5.5) are described in separate MICAD chapters (7-10).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20synthesis)]

The synthesis of cMBP was described previously (4). Briefly, the cMBP-GGG peptide was synthesized using Fmoc chemistry, with a purity of 90%.The GGG was linked to the C-terminal of the cBMP peptide. The ^125^I labeling of cMBP-GGG was done by the chloramine T method, and the reaction was terminated with sodium bisulfite. The radiochemical purity of the labeled compound was reported to be between 90% and 95% at 24 h after the labeling as determined with instant-thin layer chromatography (ITLC). The stability of ^125^I-cMBP in human serum was reported to be 90% at 1 h and 88% at 4 h as determined with ITLC.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed]

Using human glioblastoma U87MG cells, the 50% inhibitory concentration of cMBP-GGG was determined to be 65 nM (6). In a blocking study, the cells were exposed to ^125^I-cMBP-GGG (2 pmol) in the presence of excess unlabeled cMBP-GGG (1 nmol), and a significant (P = 0.001) reduction in cellular binding of the radiochemical was observed compared to controls (6). Also, a peptide containing amino acids similar to the cMBP, but in a scrambled order, had no effect on the binding of ^125^I-cMBP to the cells. Almost no ^125^I-cMBP-GGG was internalized by the cells as determined with cell internalization studies (6).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cMBP-GGG-Cy5.5+rodentia)]

The biodistribution of ^125^I-cMBP-GGG was studied in mice (n = 5 animals/time point) bearing U87MG cell xenograft tumors (6). The animals were injected with the radiochemical through the tail vein and euthanized at predetermined time points from 30 min to 24 h after the treatment. Tissues and organs of interest were subsequently removed from the animals; accumulated radioactivity was measured in a gamma counter, and the accumulated radioactivity data was presented as percent of injected dose per gram tissue (% ID/g). A high uptake of radioactivity by the pancreas was reported (20.00 ± 2.77% ID/g at 30 min, 10.13 ± 3.45% ID/g at 6 h, and 0.37 ± 0.07% ID/g at 24 h). The tumor uptake was 6.53 ± 2.29% ID/g at 30 min and decreased to 0.08 ± 0.02% ID/g by 24 h. A high uptake of the label by the kidneys was also observed (27.54 ± 5.11% ID/g at 30 min, 6.18 ± 1.92% ID/g at 6 h, and 0.22 ± 0.001% ID/g at 24 h). All other organs showed a similar distribution of radioactivity at the different time points (for details please see Table 1 of Kim and Park, et al. (6). In the same study, by comparison, the biodistribution of 125I-cBMP in the pancreas, kidneys and the tumor was reported to be 47.28 ± 4.39, 17.18 ± 1.12 and 9.3 ± 0.78%ID/g at 30 min after treatment.The tumor/blood ratio was reported to be 2.94 at 4 h after treatment with the radiolabel. Because of the high uptake of ^125^I-cMBP-GGG by the pancreas, the expression of c-Met in this organ was investigated with reverse-transcriptase polymerase chain reaction. A low expression of c-Met was observed in the pancreas, indicating that the uptake of ^125^I-cMBP-GGG by this organ was not c-Met–mediated, and accumulation of label in this organ was due to non-specific uptake. No blocking studies were reported.

From these studies, the investigators concluded that although ^125^I-cMBP-GGG was taken up by c-Met–expressing tumors, it was not a suitable imaging agent because it generated a high background due to accumulation in other tissue and organs of the animals (6).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cMBP-GGG-Cy5.5+Non-Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cMBP-GGG-Cy5.5+Non-Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cMBP-GGG-Cy5.5+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimer]

No information is currently available.

## References

1 Naran S., Zhang X., Hughes S.J. (2009). Inhibition of HGF/MET as therapy for malignancy. Expert Opin Ther Targets.
2 Abounader R., Laterra J. (2005). Scatter factor/hepatocyte growth factor in brain tumor growth and angiogenesis. Neuro Oncol.
3 Birchmeier C., Birchmeier W., Gherardi E., Vande Woude G.F. (2003). Met, metastasis, motility and more. Nat Rev Mol Cell Biol.
4 Kim E.M., Park E.H., Cheong S.J., Lee C.M., Jeong H.J., Kim D.W., Lim S.T., Sohn M.H. (2009). In vivo imaging of mesenchymal-epithelial transition factor (c-Met) expression using an optical imaging system. Bioconjug Chem.
5 Kim K., Hur Y., Ryu E.K., Rhim J.H., Choi C.Y., Baek C.M., Lee J.H., Chung J. (2007). A neutralizable epitope is induced on HGF upon its interaction with its receptor cMet. Biochem Biophys Res Commun.
6 Kim E.M., Park E.H., Cheong S.J., Lee C.M., Kim D.W., Jeong H.J., Lim S.T., Sohn M.H., Kim K., Chung J. (2009). Characterization, biodistribution and small-animal SPECT of I-125-labeled c-Met binding peptide in mice bearing c-Met receptor tyrosine kinase-positive tumor xenografts. Nucl Med Biol.
7 Chopra, A., 125I labeled mesenchymal-epithelial transition factor binding peptide [125I-cMBP]. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
8 Chopra, A., 125I labeled mesenchymal-epithelial transition factor binding peptide-8-aminooctanoic acid linker. [125I-cMBP-AOC]. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
9 Chopra, A., Mesenchymal-epithelial transition factor binding peptide-Gly-Gly-Gly-conjugated to Cy5.5 [cMBP-GGG-Cy5.5]. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
10 Chopra, A., Mesenchymal-epithelial transition factor binding peptide with an 8-aminooctanoic acid linker conjugated to Cy5.5. [cMBP-AOC-Cy5.5]. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.